# [^11^C]10-Methoxy-5-(2-propenyl)-2,5-dihydro-2,2,4-trimethyl-1H-[1]benzopyrano[3,4-f]quinoline

Chemical name: | [^11^C]10-Methoxy-5-(2-propenyl)-2,5-dihydro-2,2,4-trimethyl-1H-[1]benzopyrano[3,4-f]quinoline
Abbreviated name: | [^11^C]AL-348
Synonym:
Agent Category: | Compound
Target: | Glucocorticoid receptor
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AL+348)]

Synthetic oral glucocorticoids (GC) mediate their effects through GC receptors (GR) that are located in cytoplasm of the cell and are known to be widely distributed in all tissues. GCs such as dexamethesone and prednisolone are effective anti-inflammatory agents and are often used to treat inflammation of the muscular, intestinal, dermatological, and respiratory systems (1, 2). GCs are also used for the treatment of neuropsychodepression mediated through the hypothalamic-pituitary-adrenocortical (HPA) axis because GRs are believed to play a major role in the development of anxiety and depression (3). Also, it is well established that these tissues have a very high concentration of GRs; however, because these drugs have many undesirable side effects on the lipid and carbohydrate metabolism, such as development of osteoporosis, water retention, etc., investigators are constantly searching for new GCs (4).

It has also been reported that GR levels in the HPA are increased during episodes of anxiety or depression, and the concentration of this receptor is reduced when the individual returns to normal or low-anxiety behavior (5). To understand the regulation and functioning of the HPA axis, investigators have developed and evaluated steroid GC radiotracers labeled with fluoride (^18^F) or carbon (^11^C) to understand the activity and function of the GR system using positron emission tomography (PET) under in vivo conditions. However, studies with these radiochemicals have had limited success because the radiotracers were either metabolically unstable, had little penetration of the blood–brain barrier, and/or exhibited high nonspecific binding (6). As an alternative, some non-steroidal GR ligands respectively based on N-arylpyrazolo, dibenzenyl aniline, or benzopyrano-quinoline compounds were synthesized to study the GR system (7). Among the benzopyrano-quinoline derivatives, 10-methoxy-5-(2-propenyl)-2,5-dihydro-2,2,4-trimethyl-1H-[1]benzopyrano[3,4-f]quinoline (AL-438) was reported to have a high specificity and affinity for the GR under in vitro conditions (8). In another study the anti-inflammatory activity of AL-438 was demonstrated in a rodent model (8). On the basis of these observations, Wuest et al. labeled AL-438 with ^11^C to yield [^11^C]AL-438 and used the radiotracer for non-invasive PET imaging of brain GR in rats (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11c+AL+438)]

AL-438 was synthesized with a tetracyclic lactone as the starting material as detailed by Wuest et al. (9). The final yield of AL-438 was reported to be 73%. To radiolabel AL-438, ^11^C-methyl iodide was prepared according to the procedure of Crouzel et al. (10). The sodium salt of AL-438 in 5 N sodium hydroxide and N,N-dimethylformamide was mixed with the ^11^C-methyl iodide in a reaction vessel under a stream of nitrogen at -20°C. The reaction vessel was then sealed and heated for 5 min at 100°C. The labeled product was purified with reverse-phase high-performance liquid chromatography on a C-18 column, and the eluted product was diluted in water. The water-solubalized product was loaded onto a C-18 Sea-Pak Light cartridge, and the cartridge was washed with water. Bound [^11^C]AL-438 was eluted from the cartridge in 5% ethanol and formulated in 0.9% saline. The radiochemical yield of the labeling process was 30 ± 4% (decay corrected), with a specific activity of 10–15 GBq/μmol (0.27–0.40 Ci/μmol) at the end of synthesis (~35 min). The radiochemical purity of the labeled compound was >95%. Stability of the formulated radiotracer was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11c+AL+438+in+vitro)]

The receptor binding characteristics of AL-438 were determined with an indirect receptor binding assay with insect SF21 cells expressing either the GR or the progesterone receptor (PR) as described by Kym et al. (8) The inhibition constant (K_i_) of AL-438 was reported to be 2.5 ± 0.5 nM with 94 ± 2% efficiency compared with dexamethasone. Using the same assay, the K_i_ of AL-438 was determined to be 1,790 ± 480 nM for the PR, suggesting that AL-438 had a high specificity for the GR.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11c+AL+438+rodentia)]

The biodistribution of [^11^C]AL-438 was studied in corticosterone-treated (for competition studies) and normal male Wistar rats by a bolus injection of the radiotracer (9). The animals (n = 4 per group) were killed 5 and 60 min postinjection (p.i.), and the various tissues, selected parts and the rest of the brain, and the major organs were harvested to determine accumulated radioactivity. The amount of radioactivity in the blood reached its maximum at 5 min p.i. (0.52 ± 0.10% injected dose/gram tissue (% ID/g)) and remained relatively constant thereafter. The adrenal glands, which are rich in GR, showed the highest amount of tracer accumulation at 5 min (7.63 ± 1.38% ID/g), and these levels decreased to 4.40 ± 1.07% ID/g at 60 min. Compared with other tissues such as muscle, testis, and spleen, the accumulation of radioactivity was relatively higher in the liver (2.65 ± 0.38% ID/g), pancreas (2.79 ± 0.55% ID/g), brown fat (5.22 ± 2.50% ID/g), and the pituitary gland (2.49 ± 0.69% ID/g) 5 min p.i. In general, most organs showed little change in radiotracer incorporation between 5 and 60 min. The non–steroid-labeled compound crossed the blood–brain barrier because at 5 min p.i. it was found to be accumulated in the cerebellum (1.39 ± 0.37% ID/g), cortex (1.67 ± 0.32% ID/g), and the hippocampus (1.30 ± 0.34% ID/g). By 60 min the radioactivity had washed out from these parts of the brain and was reported to be between 0.52 ± 0.06 and 0.61 ± 0.09% ID/g.

To investigate the specificity of [^11^C]AL-438 to bind the GR, the animals were pretreated with corticosterone and injected with the tracer (9). The various tissue and organs were harvested from the rats at the two time points as detailed above. The investigators reported no change in the amount of radioactivity that bound to the adrenal glands, the thymus, the pituitary, the cortex, or cerebellum.

PET imaging was performed on a rat after injection of [^11^C]AL-438 through the tail vein (9). Various regions of the brain were reported to be clearly visible, which was consistent with the brain biodistribution data with the radiotracer. After a high uptake of the label during the initial period, a steady decline in accumulation of the radioactivity was noted.

On the basis of the incorporated radioactivity in normal and in corticosterone-treated animals, the investigators concluded that, although [^11^C]AL-438 crossed the blood–brain barrier, it bound non-specifically to brain tissue probably because the compound is lipophilic and therefore the tracer uptake was not GR-mediated.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11c+AL+438+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11c+AL+438+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Elmore S.W., Pratt J.K., Coghlan M.J., Mao Y., Green B.E., Anderson D.D., Stashko M.A., Lin C.W., Falls D., Nakane M., Miller L., Tyree C.M., Miner J.N., Lane B. (2004). Differentiation of in vitro transcriptional repression and activation profiles of selective glucocorticoid modulators. Bioorg Med Chem Lett.
2 Rhen T., Cidlowski J.A. (2005). Antiinflammatory action of glucocorticoids--new mechanisms for old drugs. N Engl J Med.
3 Pariante C.M., Lightman S.L. (2008). The HPA axis in major depression: classical theories and new developments. Trends Neurosci.
4 Schacke H., Docke W.D., Asadullah K. (2002). Mechanisms involved in the side effects of glucocorticoids. Pharmacol Ther.
5 Rozeboom A.M., Akil H., Seasholtz A.F. (2007). Mineralocorticoid receptor overexpression in forebrain decreases anxiety-like behavior and alters the stress response in mice. Proc Natl Acad Sci U S A.
6 Steiniger B., Kniess T., Bergmann R., Pietzsch J., Wuest F.R. (2008). Radiolabeled glucocorticoids as molecular probes for imaging brain glucocorticoid receptors by means of positron emission tomography (PET). Mini Rev Med Chem.
7 Buijsman R.C., Hermkens P.H., van Rijn R.D., Stock H.T., Teerhuis N.M. (2005). Non-steroidal steroid receptor modulators. Curr Med Chem.
8 Kym P.R., Kort M.E., Coghlan M.J., Moore J.L., Tang R., Ratajczyk J.D., Larson D.P., Elmore S.W., Pratt J.K., Stashko M.A., Falls H.D., Lin C.W., Nakane M., Miller L., Tyree C.M., Miner J.N., Jacobson P.B., Wilcox D.M., Nguyen P., Lane B.C. (2003). Nonsteroidal selective glucocorticoid modulators: the effect of C-10 substitution on receptor selectivity and functional potency of 5-allyl-2,5-dihydro-2,2,4-trimethyl-1H-[1]benzopyrano[3,4-f]quinolines. J Med Chem.
9 Wuest F., Kniess T., Bergmann R., Henry B., Pietzsch J. (2007). Synthesis and radiopharmacological characterization of [11C]AL-438 as a nonsteroidal ligand for imaging brain glucocorticoid receptors. Bioorg Med Chem Lett.
10 Crouzel C., Langstrom B., Pike V.W., Coenen H.H. (1987). Recommendations fpr a practical production of [ ^ 11 ^ C]methyl iodide. Applied Radiation and Isotopes.